# N-(5-Fluoro-2-phenoxyphenyl)-N-(2-[^18^F]fluoroethyl-5-methoxybenzyl)acetamide

Chemical name: | N-(5-Fluoro-2-phenoxyphenyl)-N-(2-[^18^F]fluoroethyl-5-methoxybenzyl)acetamide
Abbreviated name:
Synonym: | [^18^F]FEDAA1106
Agent Category: | Compound
Target: | Peripheral-type benzodiazepine receptor (PBR)
Target Category: | Receptor binding
Method of detection: | PET
Source of signal: | ^18^F
Activation: | No
Studies: | - In vitro; - Rodents; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEDAA1106%5BAll%20Fields%5D)]

Benzodiazepines, such as diazepam, are potent psychoactive drugs used for their sedative and anxiolytic properties (1, 2). There are two types of benzodiazepine receptors, which have been designated as the central and peripheral benzodiazepine receptors. The central benzodiazepine receptor (CBR) is found exclusively in the central nervous system on the membranes of neurons and is coupled to the γ-aminobutyric acid receptor/chloride channel (3). In contrast, the peripheral benzodiazepine receptor (PBR) is a mitochondrial protein found in brain and peripheral tissues (adrenal gland, heart, lung, kidney, and testis) (4). The brain has lower levels of PBRs than do the peripheral tissues. Both glial cells and macrophages contain high levels of PBRs (5-7). Increased PBR expression after brain injury or neuroinflammation is associated with microglial activation, such as occurs with the neuronal damage accompanying several neurodegenerative diseases, including Alzheimer’s disease, Wernicke’s encephalopathy, multiple sclerosis, and epilepsy.

PBRs have been studied in vivo by positron emission tomography (PET) using [^11^C]PK11195, an isoquinoline carboxamide with specific PBR-antagonistic activity. [^11^C]PK11195 is being developed as a PET agent for non-invasive studies of microglia and macrophage activation in the brain, lung, and heart. However, accumulation of this tracer in the brain is limited. N-(2,5-Dimethoxybenzyl)-N-(5-fluoro-2-phenoxyphenyl)acetamide (DAA1106) was found to be a selective agonist for studying PBRs in the central nervous system (8, 9). DAA1106 was reported to have a higher affinity for PBRs in mitochondrial fractions of rat and monkey brains than did PK11195 (8, 9). Therefore, both tracers are able to cross the normal cell membrane to reach the mitochondrial receptor sites. [^11^C]DAA1106 has been studied as a PET agent for the non-invasive study of microglia and macrophage activation in the brain. [^11^C]DAA1106 binding was 3-fold higher than [^11^C]PK11195 binding in the monkey occipital cortex (9). N-(5-Fluoro-2-phenoxyphenyl)-N-(2-[^18^F]fluoroethyl-5-methoxybenzyl)acetamide ([^18^F]FEDAA1106), a fluoroethyl analog of DA1106, is being developed as a potential PET ligand with highly selective and specific binding to PBR.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEDAA1106%20and%20synthesis)]

In the report by Zhang et al. (10), [^18^F]FEDAA1106 was synthesized by alkylation of N-(5-fluoro-2-phenoxyphenyl)-N-(2-hydroxy-5-methoxybenzyl)-acetamide with 2-[^18^F]fluoroethyl bromide ([^18^F]FCH_2_CH_2_Br) in the presence of NaH. [^18^F]FCH_2_CH_2_Br was prepared by the reaction of [^18^F]F− with 2-bromoethyl triflate (BrCH_2_CH_2_OTf), using an automated system. Subsequent high-performance liquid chromatography (HPLC) separation gave a radiochemical purity >98%. The specific activity was 120 GBq/μmol (3.2 Ci/μmol) at end of synthesis with 12 ± 4% radiochemical yield. Total synthesis time was 50 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEDAA1106%20and%20in%20vitro)]

In vitro [^11^C]DAA1106 PBR-binding studies showed IC_50_ values of 0.77, 1.62 and 8.26 nM for FEDAA1106, DAA1106, and PK11195, respectively (10). All three compounds had little affinity for CBRs as measured by [^11^C]flumazenil binding assays. Hence, FEDAA1106 is 10-fold more potent than PK11195. In vitro binding studies of [^3^H]DAA1106 produced K_d_ values of 0.12 ± 0.03 and 0.43 ± 0.04 nM for mitochondrial fractions of rat and monkey cerebral cortex, respectively (9). The PBR B_max_ values were 161.03 ± 5.8, and 701 ± 70 fmol/mg protein for mitochondrial fractions of rat and monkey cerebral cortex, respectively. Regional distribution of [^3^H]DAA1106 in mitochondrial fractions of the rat brain revealed that the olfactory bulb has the highest B_max_ (>400 fmol/mg protein), followed by the cerebellum, cerebral cortex, hypothalamus, striatum, hippocampus, and thalamus. This pattern of DAA1106 binding in the brain was later confirmed by in vitro autoradiographic studies using [^11^C]DAA1106 in rats.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEDAA1106%20and%20rodentia)]

Zhang et al. (10) reported ex vivo autoradiographic accumulation of [^18^F]FEDAA1106 in all brain regions at 30 min after injection. The highest uptake was in the olfactory bulb (0.8 fmol/mm^2^), followed by the cerebellum (0.37 fmol/mm^2^) and cerebral cortex (0.2 fmol/mm^2^). Coadiministration of unlabeled DAA1106 decreased the accumulation in all brain regions with the most significant reduction in the olfactory bulb (80% inhibition) followed by the other regions (40-60% inhibition). Almost all of the radioactivity in the brain was intact [^18^F]FEDAA1106 at 30 min after injection. Because the target receptor is in the mitochondria, the compound has to cross the blood-brain barrier and the cell membrane readily to reach its target. About 29% of radioactivity in the plasma was intact [^18^F]FEDAA1106 at 30 min after injection.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEDAA1106%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publications are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEDAA1106%20and%20%28primate%20not%20human%29)]

Zhang et al. (11) reported PET studies of [^18^F]FEDAA1106, [^11^C]DAA1106, and [^11^C]R-PK11195 in monkey brain. [^18^F]FEDAA1106 displayed high uptake in the occipital cortex, a region rich in PBRs. The radioactivity level of [^18^F]FEDAA1106 in monkey brain was 1.5 times higher than that of [^11^C]DAA1106 and 6 times higher than that of [^11^C]R-PK11195. The accumulation of [^18^F]FEDAA1106 was inhibited significantly by pretreatment of PK11195 (5 mg/kg) or DAA1106 (1 mg/kg), indicating that the binding of [^18^F]FEDAA1106 in the monkey brain was mainly attributable to PBRs. Metabolite analysis in the plasma revealed that [^18^F]FEDAA1106 was metabolized by debenzylation to a polar product, which was not detected in the mouse brain. About 50% of radioactivity in the plasma was intact [^18^F]FEDAA1106 at 30 min after injection.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=FEDAA1106%20and%20human)]

Fujimura et al. (12) reported PET studies with [^18^F]FEDAA1106 in 7 healthy men. Regional distribution in the brain was assessed by binding potential (BP), which was calculated by nonlinear least-squares (NLS) analysis based on the two-tissue compartment model, and distribution volume (DV), which was estimated by NLS, Logan plot, and multilinear analysis methods. The DVs estimated with each of the methods were significantly correlated. There was also significant correlation of BP with NLS and DV with NLS, Logan plot, or multilinear analysis. The simulation studies indicated that NLS is a suitable method for the estimation of [^18^F]FEDAA1106 binding to PBRs. Internal dosimetry data for [^18^F] FEDAA1106 in humans are not available in the literature.

## References

1 Mohler H., Okada T. (1977). Benzodiazepine receptor: demonstration in the central nervous system. Science.
2 Hunkeler W., Mohler H., Pieri L., Polc P., Bonetti E.P., Cumin R., Schaffner R., Haefely W. (1981). Selective antagonists of benzodiazepines. Nature.
3 Olsen R.W., Tobin A.J. (1990). Molecular biology of GABAA receptors. Faseb J.
4 Anholt R.R., Pedersen P.L., De Souza E.B., Snyder S.H. (1986). The peripheral-type benzodiazepine receptor. Localization to the mitochondrial outer membrane. J Biol Chem.
5 Jones H.A., Valind S.O., Clark I.C., Bolden G.E., Krausz T., Schofield J.B., Boobis A.R., Haslett C. (2002). Kinetics of lung macrophages monitored in vivo following particulate challenge in rabbits. Toxicol Appl Pharmacol.
6 Kuhlmann A.C., Guilarte T.R. (2000). Cellular and subcellular localization of peripheral benzodiazepine receptors after trimethyltin neurotoxicity. J Neurochem.
7 Zavala F., Lenfant M. (1987). Benzodiazepines and PK 11195 exert immunomodulating activities by binding on a specific receptor on macrophages. Ann N Y Acad Sci.
8 Okuyama S., Chaki S., Yoshikawa R., Ogawa S., Suzuki Y., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Neuropharmacological profile of peripheral benzodiazepine receptor agonists, DAA1097 and DAA1106. Life Sci.
9 Chaki S., Funakoshi T., Yoshikawa R., Okuyama S., Okubo T., Nakazato A., Nagamine M., Tomisawa K. (1999). Binding characteristics of [3H]DAA1106, a novel and selective ligand for peripheral benzodiazepine receptors. Eur J Pharmacol.
10 Zhang M.R., Maeda J., Furutsuka K., Yoshida Y., Ogawa M., Suhara T., Suzuki K. (2003). [18F]FMDAA1106 and [18F]FEDAA1106: two positron-emitter labeled ligands for peripheral benzodiazepine receptor (PBR). Bioorg Med Chem Lett.
11 Zhang M.R., Maeda J., Ogawa M., Noguchi J., Ito T., Yoshida Y., Okauchi T., Obayashi S., Suhara T., Suzuki K. (2004). Development of a new radioligand, N-(5-fluoro-2-phenoxyphenyl)-N-(2-[18F]fluoroethyl-5-methoxybenzyl)acetami de, for pet imaging of peripheral benzodiazepine receptor in primate brain. J Med Chem.
12 Fujimura Y., Ikoma Y., Yasuno F., Suhara T., Ota M., Matsumoto R., Nozaki S., Takano A., Kosaka J., Zhang M.R., Nakao R., Suzuki K., Kato N., Ito H. (2006). Quantitative Analyses of 18F-FEDAA1106 Binding to Peripheral Benzodiazepine Receptors in Living Human Brain. J Nucl Med.